# ^99m^Tc-labeled [N_4_^0^,Pro^1^,Tyr^4^]bombesin

Chemical name: | ^99m^Tc-labeled [N_4_^0^,Pro^1^,Tyr^4^]bombesin
Abbreviated name: | [^99m^Tc]Demobesin 3
Synonym:
Agent Category: | peptide
Target: | Gastrin-releasing peptide receptor (GRPR)
Target Category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=4885361), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=61677286) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2925) for more information about gastrin-releasing peptide receptor.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22bombesin%22%25GRPR%20imaging)]

^99m^Tc-labeled [N_4_^0^,Pro^1^,Tyr^4^]bombesin ([^99m^Tc]Demobesin 3) is a bombesin (BN) analog developed by Nock et al. for molecular imaging of tumors expressing gastrin-releasing peptide (GRP) receptor (GRPR) (1).

BN is an amphibian neuropeptide consisting of 14 amino acids (pGlu-Gln-Arg-Leu-Gly-Asn-Gln-Trp-Ala-Val-Gly-His-Leu-Met-NH_2_) (2, 3), and it was first isolated from frog skin in 1970 (4). The search for its mammalian counterpart led to the discovery of GRP, which consists of 27 amino acids. GRP and BN share an identical C-terminal region (-Trp-Ala-Val-Gly-His-Leu-Met-NH_2_), which is necessary for receptor binding and signal transduction (5, 6). In addition to the release of gastrin, GRP- and BN-like peptides also produce a wide range of other biological responses in diverse tissues, such as secretion of endocrine and exocrine glands, maintenance of circadian rhythm, regulation of satiety, and contraction of smooth muscles (7). They also act as potential growth factors for both normal and cancerous cells (3, 5, 6). There are four members of the BN receptor family, including three mammalian receptors: GRPR (BB_2_ or BRS2; 384 amino acids), neuromedin B receptor (NMBR, BB_1_, or BRS1; 390 amino acids), and BN-like receptor 3 (BB_3_, BRS3, or orphan; 399 amino acids) (5, 7, 8); the fourth receptor (BB_4_) has only been found in amphibians. GRPR is the only well characterized receptor of this family. GRPR is a glycosylated, 7-transmembrane, G-protein–coupled receptor that, upon binding with its ligands, gives rise to a complex cascade of intracellular reactions. It is normally found in non-neuroendocrine tissues of the breast and pancreas, and in neuroendocrine cells of the brain, gastrointestinal tract, lung, and prostate (9). Interestingly, GRPR is overexpressed in prostate cancer as well as in tumors of the breast, lung, pancreas, ovary, kidney, and gastrointestinal tract. It has been reported that GRPR is expressed at a high density in the intraepithelial neoplasia and primary carcinoma of the prostate, whereas normal prostate tissue and, in most cases, benign prostate hyperplasia are predominantly negative for GRPR (10-13).

GRPR has attracted significant interest as a target for tumor detection, tumor staging, and evaluation of tumor response to therapy (5, 6, 8, 11). A large number of BN derivatives have been developed, and they have been labeled with ^99m^Tc, ^177^Lu, ^67^Ga, and ^111^In for single-photon emission computed tomography (SPECT) and with ^64^Cu, ^68^Ga, and ^18^F for positron emission tomography. The published BN derivatives can be generally classified as truncated BN (6–14 or 7–14) or full-length BN (1-14) analogs (10, 12-18). The truncated BN analogs seem to be favorable for in vivo applications because they are usually more stable than the full-length tetradecapeptides and still bind to the GRPR adequately. However, the full-length peptides offer different labeling methods by attachment of functional groups to the amino acids 1–6. In many cases, the amino acids on positions 13 (Leu) and 14 (Met) have been replaced by unnatural amino acids (cyclohexylalanine (CyHAla) and norleucine (Nle)), and Lys has been placed on position 3 for attachment of radiolabels with reactive esters. Spacers, chelators, or radiometals have also been widely used for conjugation and for favorable kinetics (19). The BN derivatives can also be divided into agonists and antagonists (1, 20, 21). By far, most BN derivatives are agonists. Agonists are internalized into and accumulate within cells, and it has been assumed that they exhibit higher uptake by cancer cells than antagonists. However, some reports have shown that uptake of antagonists in vivo into tumor xenografts is higher than that of agonists (20, 21). Antagonists may have stronger binding for the GRPR than agonists (20, 21), and it has been suggested that antagonists may bind to all of the receptors, whereas agonists may only bind to the high affinity sites of the receptors.

An optimal BN-like radiotracer needs to meet several requirements: high affinity for GRPR, with rapid and specific tumor uptake; high hydrophilicity, with preferred renal excretion and low hepatobiliary excretion; and high stability but relatively rapid clearance from blood (6). Despite a large number of published derivatives, a valid comparison among them for the feasibility of tumor imaging is difficult because standardization between studies is lacking. Generally speaking, the majority of the radiotracers have relatively high renal and hepatic uptake, resulting in low tumor/liver and tumor/kidney ratios. Nock et al. synthesized four BN analogs, Demobesins 3–6, and labeled them with ^99m^Tc for imaging of GRPR-expressing tumors (1). The [^99m^Tc]Demobesins 3–4 were synthesized on the basis of the parent BN tetradecapeptide sequence with minor modifications, while the [^99m^Tc]Demobesins 5–6 were truncated peptides on the basis of the essential residues (the BN(7–14) motif) needed for receptor interaction. Different from [^99m^Tc]Demobesins 3 and 5, the oxidation-sensitive Met^14^ was replaced by Nle^14^ in [^99m^Tc]Demobesins 4 and 6. Their studies showed that all four BN analogs had high affinity for the human GRPR, efficiently internalized in the GRPR-expressing PC-3 cells in a time- and dose-dependent manner. The [^99m^Tc]Demobesins 3 and 4 presented high and rapid localization in the tumors with rapid clearance via the kidneys, while the [^99m^Tc]Demobesins 5 and 6 showed a lower tumor uptake and excessive hepatobiliary excretion.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=demobesin)]

The peptide Demobesin 3 was synthesized with standard 9-fluorenylmethyloxycarbonyl (Fmoc)/tert-butyl methodology on an automated synthesizer (1). The completeness of the reaction was monitored with the ninhydrin test. The sequence was Pro-Gln-Arg-Tyr-Gly-Asn-Gln-Trp-Ala-Val-Gly-His-Leu-Met-NH_2_. The synthesizing time was 2.0–2.5 h. Fmoc deprotection was achieved by treatment with piperidine in N,N-dimethylformamide (DMF). The tetraamine chelator precursor N,N’,N’’,N’’’-tetrakis(tert-butoxycarbonyl)-6-(carboxy)-1,4,8,11-tetraazaundecane (N_4_(Boc)_4_-COOH) was coupled at the N-terminal of the amino acid chain with the coupling agent o-(7-azabenzotriazol-1-yl)-N,N,N’,N’-tetramethyluronium hexafluorophosphate in the presence of N,N-diisopropylethylamine in DMF (2.5 h coupling). Removal of the lateral chain protecting groups and cleavage from the resin were performed by 3.5 h incubation in a cleavage cocktail comprising trifluoroacetic acid:anisole:1,2-ethanedithiol:H_2_O:dichloromethane (85:3:2:3:7 v/v/v/v/v). The yield of crude products was 70–80%. The products were further purified and lyophilized with 50–60% yield. The expected molecular weights were 1.84 kDa. For radiolabeling, each peptide was dissolved in acetic acid/EtOH (8/2 v/v), followed by addition of sodium citrate, pertechnetate generator eluate, and freshly prepared ethanolic SnCl_2_ solution. The mixture was left to react for 30 min at ambient temperature, and was then brought to pH 7 before purification. The purity was >96%, and the specific activity was 37 GBq/µmol (1 Ci/µmol) total peptide. The expected radiochemical impurities (^99m^TcO_4_^-^, [^99m^Tc]citrate, and ^99m^TcO_2_·xH_2_O) were detectable by <2%. The radiopeptide remained intact within the open labeling reaction vial for at least 6 h after labeling. A similar procedure was applied for preparation of the corresponding [^99m^Tc/^99g^Tc]peptide with [^99g^Tc]NH_4_TcO_4_ as the ^99g^Tc source. Radioiodination of [Tyr^4^]BN was performed as described previously (22).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=demobesin)]

The binding affinity of Demobesin 3 was determined with competition binding assay in PC-3 cells (1). [^125^I-Tyr^4^]BN was used as the specific radioligand for GRPR, while [Tyr^4^]BN was used as the reference. Demobesin 3 peptide was able to displace the [^125^I-Tyr^4^]BN from the BN binding sites in PC-3 cell membranes in a monophasic and dose-dependent manner. The 50% inhibitory concentration (IC_50_) value was 0.06 ± 0.04 nmol, and was comparable or better than the respective value of [Tyr^4^]BN (0.85 ± 0.29 nmol). The GRPR affinity of Demobesin 3 was similar to that of Demobesin 5, but slightly higher than that of Demobesin 4 and its truncated counterpart Demobesin 6 with substitution of the Met^14^ by the Nle^14^.

The selective affinity of Demobesin 3 for each of the three human BN receptor subtypes was studied in surgical samples of human tumors (1). The specimens included NMBR-expressing ileal carcinoids, GRPR-expressing prostate cancer, and BB_3_-expressing lung carcinoids (n = 2/tumor subtype). Receptor autoradiography and IC_50_ measurement showed that Demobesin 3, similar to Demobesins 4-6, had high affinity for the GRPR (mean IC_50_ = 0.47), less affinity for the NMBR (mean IC_50_ = 1.6), and no affinity for the BB_3_ (mean IC_50_ = >100). Again, as compared with Nle^14^-containing Demobesins 4 and 6, Demobesins 3 and 5 exhibited slightly high affinity for the GRPR.

The internalization of [^99m^Tc]Demobesin 3 was determined in PC-3 cells (1). Rapid internalization was observed, reaching a 75% plateau within the first 30 min and remaining at this level for up to 2 h of incubation. The internalization was negligible in the presence of 1 µmol [Tyr^4^]BN, suggesting a receptor-mediated process.

The metabolic fate of [^99m^Tc]Demobesin 3 was studied by incubation of the radiopeptide in murine plasma at 37°C (1). It has been shown that the radiopeptide catabolism was slow in mouse plasma during the initial critical time intervals, with >90% radiopeptide remaining intact within 10 min incubation, and with 60–80% and 40–60% intact within 1 h and 2 h incubation, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=demobesin)]

Biodistribution studies of the [^99m^Tc]Demobesin 3 were conducted in female nu/nu mice bearing PC-3 tumor xenografts (1). [^99m^Tc]Demobesin 3 was injected as a bolus containing 148–185 GBq (4–5 µCi, ~10 pmol total peptide) through the tail vein of each mouse. Animals were euthanized at 1, 4, and 24 h time intervals (n = 4–5 mice/group). An additional set of four animals was intravenously administered 100 µg [Tyr^4^]BN along with the radiopeptide (blocked animals). These animals were euthanized at 4 h after injection.

[^99m^Tc]Demobesin 3, similar to [^99m^Tc]Demobesins 4-6, was rapidly cleared via the liver and the kidneys, showing low background radioactivity. While [^99m^Tc]Demobesins 3 and 4 were excreted predominantly via the kidneys, the truncated and more lipophilic [^99m^Tc]Demobesins 5 and 6 showed a high percentage of hepatobiliary excretion. Uptake of the radiopeptides in the PC-3 xenograft was high, especially for the [^99m^Tc]Demobesins 3 and 4 (9–11% injected dose per gram tissue (ID/g) at 1 h after injection), remaining high (7–9% ID/g) at 4 h after injection. The uptake values were greatly reduced by co-injection of the [Tyr^4^]BN, being only 0.2–0.8% ID/g at 4 h after injection. Similarly, uptake of all four radiopeptides in the pancreas was very high and declined slowly over 24 h after injection. Treatment with [Tyr^4^]BN caused a >97% drop in the pancreas uptake at 4 h after injection. The intestinal accumulation of [^99m^Tc]Demobesins 3 and 4 was relatively low and could be blocked with co-injection of the [Tyr^4^]BN (by 85% at 4 h after injection). In contrast, the intestinal uptake of [^99m^Tc]Demobesins 5 and 6 was much higher and was not blocked with [Tyr^4^]BN treatment. The increased uptake of [^99m^Tc]Demobesins 5 and 6 in the intestine might be due to their higher lipophilicity originating from the extra benzyl group of the spacer as well as the lack of the polar and hydrophilic Arg^3^ and Tyr^4^ residues present in the [^99m^Tc]Demobesins 3 and 4.

Analysis of the urine collected 30 min after injection of the [^99m^Tc]Demobesins 3–6 revealed that all four radiopeptides excreted into the urine completely converted to more hydrophilic metabolites. The [^99m^Tc]Demobesins 3 and 4 produced one hydrophilic metabolite (I), whereas the truncated [^99m^Tc]Demobesins 5 and 6 generated two metabolic species (II and III). Metabolite I was distinct from and more hydrophilic than metabolites II and III. It has been assumed that these metabolic products were generated by cleavage of the amide bond(s) either within the peptide chain or between the metal chelate and the peptide, rather than by in vivo breakdown of the metal chelate (1, 20).

Imaging studies were performed in two PC-3 xenograft-bearing mice with tail vein injection of 18.5–37 MBq (0.5–1 mCi) [^99m^Tc]Demobesin 3 alone in one mouse and together with 100 µg [Tyr^4^]BN in another mouse (blocked). The mice were euthanized and imaged at 90 min after injection. In the first mouse the tumor was clearly delineated with a very low background activity, while in the blocked mouse the tumor was not detectable by the camera.

In summary, all four radiopeptides showed high affinity for the human GRPR both in GRPR-positive PC-3 cells and in human tumor samples. Internalization of the four radiopeptides was efficient and rapid in the PC-3 cells, but they were distinct for their in vivo profiles in xenograft-bearing mice. In comparison to the antagonist-based [^99m^Tc]Demobesin 1 (http://www.ncbi.nlm.nih.gov/bookshelf/corehtml/pmc/homepages/bookshelf/micad.html) (20, 21), much higher internalization efficiency of the agonist-based [^99m^Tc]Demobesins 3–6 did not translate into a higher tumor and target-organ accumulation in vivo.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Nock B.A., Nikolopoulou A., Galanis A., Cordopatis P., Waser B., Reubi J.C., Maina T. (2005). Potent bombesin-like peptides for GRP-receptor targeting of tumors with 99mTc: a preclinical study. J Med Chem.
2 Maina T., Nock B.A., Zhang H., Nikolopoulou A., Waser B., Reubi J.C., Maecke H.R. (2005). Species differences of bombesin analog interactions with GRP-R define the choice of animal models in the development of GRP-R-targeting drugs. J Nucl Med.
3 Smith C.J., Volkert W.A., Hoffman T.J. (2003). Gastrin releasing peptide (GRP) receptor targeted radiopharmaceuticals: a concise update. Nucl Med Biol.
4 Erspamer V., Erpamer G.F., Inselvini M. (1970). Some pharmacological actions of alytesin and bombesin. J Pharm Pharmacol.
5 Smith C.J., Volkert W.A., Hoffman T.J. (2005). Radiolabeled peptide conjugates for targeting of the bombesin receptor superfamily subtypes. Nucl Med Biol.
6 Ananias H.J., de Jong I.J., Dierckx R.A., van de Wiele C., Helfrich W., Elsinga P.H. (2008). Nuclear imaging of prostate cancer with gastrin-releasing-peptide-receptor targeted radiopharmaceuticals. Curr Pharm Des.
7 Ischia J., Patel O., Shulkes A., Baldwin G.S. (2009). Gastrin-releasing peptide: different forms, different functions. Biofactors.
8 Maina T., Nock B., Mather S. (2006). Targeting prostate cancer with radiolabelled bombesins. Cancer Imaging.
9 Weber H.C. (2009). Regulation and signaling of human bombesin receptors and their biological effects. Curr Opin Endocrinol Diabetes Obes.
10 Yang Y.S., Zhang X., Xiong Z., Chen X. (2006). Comparative in vitro and in vivo evaluation of two 64Cu-labeled bombesin analogs in a mouse model of human prostate adenocarcinoma. Nucl Med Biol.
11 Liu S., Edwards D.S., Barrett J.A. (1997). 99mTc labeling of highly potent small peptides. Bioconjug Chem.
12 Zhang X., Cai W., Cao F., Schreibmann E., Wu Y., Wu J.C., Xing L., Chen X. (2006). 18F-labeled bombesin analogs for targeting GRP receptor-expressing prostate cancer. J Nucl Med.
13 Schroeder R.P., van Weerden W.M., Bangma C., Krenning E.P., de Jong M. (2009). Peptide receptor imaging of prostate cancer with radiolabelled bombesin analogues. Methods.
14 Chen X., Park R., Hou Y., Tohme M., Shahinian A.H., Bading J.R., Conti P.S. (2004). microPET and autoradiographic imaging of GRP receptor expression with 64Cu-DOTA-[Lys3]bombesin in human prostate adenocarcinoma xenografts. J Nucl Med.
15 Hohne A., Mu L., Honer M., Schubiger P.A., Ametamey S.M., Graham K., Stellfeld T., Borkowski S., Berndorff D., Klar U., Voigtmann U., Cyr J.E., Friebe M., Dinkelborg L., Srinivasan A. (2008). Synthesis, 18F-labeling, and in vitro and in vivo studies of bombesin peptides modified with silicon-based building blocks. Bioconjug Chem.
16 Li Z.B., Wu Z., Chen K., Ryu E.K., Chen X. (2008). 18F-labeled BBN-RGD heterodimer for prostate cancer imaging. J Nucl Med.
17 Prasanphanich A.F., Retzloff L., Lane S.R., Nanda P.K., Sieckman G.L., Rold T.L., Ma L., Figueroa S.D., Sublett S.V., Hoffman T.J., Smith C.J. (2009). In vitro and in vivo analysis of [(64)Cu-NO2A-8-Aoc-BBN(7-14)NH(2)]: a site-directed radiopharmaceutical for positron-emission tomography imaging of T-47D human breast cancer tumors. Nucl Med Biol.
18 Santos-Cuevas C.L., Ferro-Flores G., Arteaga de Murphy C., Ramirez Fde M., Luna-Gutierrez M.A., Pedraza-Lopez M., Garcia-Becerra R., Ordaz-Rosado D. (2009). Design, preparation, in vitro and in vivo evaluation of (99m)Tc-N2S2-Tat(49-57)-bombesin: a target-specific hybrid radiopharmaceutical. Int J Pharm.
19 Fragogeorgi, E.A., C. Zikos, E. Gourni, P. Bouziotis, M. Paravatou-Petsotas, G. Loudos, N. Mitsokapas, S. Xanthopoulos, M. Mavri-Vavayanni, E. Livaniou, A.D. Varvarigou, and S.C. Archimandritis, Spacer Site Modifications for the Improvement of the in Vitro and in Vivo Binding Properties of (99m)Tc-N(3)S-X-Bombesin[2-14] Derivatives. Bioconjug Chem, 2009
20 Nock B., Nikolopoulou A., Chiotellis E., Loudos G., Maintas D., Reubi J.C., Maina T. (2003). [99mTc]Demobesin 1, a novel potent bombesin analogue for GRP receptor-targeted tumour imaging. Eur J Nucl Med Mol Imaging.
21 Cescato R., Maina T., Nock B., Nikolopoulou A., Charalambidis D., Piccand V., Reubi J.C. (2008). Bombesin receptor antagonists may be preferable to agonists for tumor targeting. J Nucl Med.
22 Mantey S., Frucht H., Coy D.H., Jensen R.T. (1993). Characterization of bombesin receptors using a novel, potent, radiolabeled antagonist that distinguishes bombesin receptor subtypes. Mol Pharmacol.